# Microbubble-conjugated vascular endothelial growth factor receptor 2 monoclonal antibody

Chemical name: | Microbubble-conjugated vascular endothelial growth factor receptor 2 monoclonal antibody
Abbreviated name: | Microbubble-conjugated VEGFR2 mAb
Synonym: | Ultrasound contrast agent (UCA) conjugated with an anti-VEGFR2 monoclonal antibody
Agent Category: | Monoclonal antibody
Target: | Vascular endothelial growth factor receptor 2 (VEGFR2)
Target Category: | Antibody-ligand binding
Method of detection: | Ultrasound
Source of signal: | Microbubbles
Activation: | No
Studies: | - Rodents | Click here for the protein and mRNA (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=56385329) sequence of human VEGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2+ultrasonography)]

There are three known receptors for the vascular endothelial growth factor (VEGF), designated as VEGF receptor 1 (VEGFR1), receptor 2 (VEGFR2), and receptor 3 (VEGFR3). During embryogenesis these receptors are involved in vasculogenesis, angiogenesis, and lymphangiogenesis (1, 2). Among the three receptors, VEGFR2 was shown to be the primary signal transducer for angiogenesis and the development of pathological conditions such as cancer and diabetic retinopathy. It has been shown that VEGFR2 is expressed mainly in the endothelial cells, and the expression is upregulated in the tumor vasculature (2-4). Thus the inhibition of VEGFR2 activity and its downstream signaling are important targets for the treatment of diseases involving angiogenesis. A variety of VEGFR2 antagonists, including kinase inhibitors and neutralizing antibodies, are now in clinical trials (http://clinicaltrials.gov/ct/search?term=VEGFR2+inhibitors) for the diagnosis and treatment of these pathologies. For such therapies to be successful, it is important to select patients who are most likely to respond to the treatment and to be able to rapidly evaluate the response after initiation of therapy. Resection of the tumor(s), followed by immunohistochemical analysis, is an invasive technique and may not always yield expected results because of sampling bias or errors (5, 6). Also, methods based on tumor size measurement by cross-sectional imaging are used to determine treatment response, but because of insensitivity of the method the size changes may not be detected, especially immediately after a treatment, or the effects may not be apparent because of a delayed response. This can lead to an inaccurate interpretation of results and conclusions, and the development of a suboptimal therapeutic regimen (7, 8).

Lyshchik et al. suggested that molecular ultrasonography could be a potential technique for the non-invasive investigation of tumor vasculature because the information on molecular and cellular profiles of the endothelial cells available with this technique can be correlated to data on the perfusion and microvascular blood volume obtained during the procedure (9). Microbubble (MB) ultrasound contrast agents (UCAs) conjugated to either peptides or antibodies against integrins have previously been used for the non-invasive assessment and imaging of angiogenesis (10, 11). However, because of the low-resolution images obtained during these studies, an accurate assessment of angiogenesis could not be made with these studies. Lyshchik et al. developed a UCA by conjugating a commercially available lyophilized MB preparation with biotinylated monoclonal antibodies (mAb) against VEGFR2 (9). The VEGFR2-conjugated UCA was used to investigate the expression of VEGFR2 on the vascular endothelium in a breast cancer murine model.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2+UCA+synthesis)]

The UCA was prepared with a commercially available (http://www.visualsonics.com/products/products_micromarker.htm) MB kit specifically designed to conjugate the anti-VEGFR2 mAb, as recommended by the manufacturer (9). The UCA has streptavidin chemically linked to the phospholipid shell of the MB through a polyethylene glycol spacer and was designed to obtain maximum saturation of the MB surface with an antibody, leaving a minimal amount of free antibody in solution. The preparation was available to the investigators as a vial of lyophilized powder containing 9.2 × 10^8^ dry, streptavidin-coated MBs that were filled with a mixture of nitrogen and perfluorobutane. No information regarding the number of antibody molecules linked to each MB were provided in the publication.

The dry UCA was resuspended in sterile saline and ~200 nmol of either biotinylated anti-mouse VEGFR2 mAb (http://www.ebioscience.com/ebioscience/specs/pdf/antibody_13/13-5821.pdf) or immunoglobulin G isotype control (http://www.ebioscience.com/ebioscience/specs/pdf/antibody_13/13-4732.pdf) were added to the solution to produce a VEGFR2-targeted UCA or a control UCA, respectively. The opacity of the UCA was monitored visually to ensure no MB was destroyed. The storage conditions of the UCA after preparation, until used, were not provided by the investigators.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2+sonography+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2+UCA+rodentia)]

The VEGFR2-targeted UCA was evaluated in athymic nu/nu mice. Mice (n = 5 in each group) were injected with murine 4T1 (http://www.atcc.org/common/catalog/numSearch/numResults.cfm?atccNum=CRL-2539) and 67NR (http://cancerres.aacrjournals.org/cgi/reprint/52/6/1399) breast cancer cells, respectively, in the hind limbs (9). The tumors were allowed to grow 6 to 8 days until they reached a maximum diameter of 5 to 8 mm. To reduce the chances of injection sequence bias, the mice were administered VEGFR2-targeted UCA or the control UCA in random order with a 30-min interval. The 4T1 tumors showed a moderate intensity signal of 15 ± 3.4 dB, and the control tumors had a mild signal intensity of 7 ± 1.6 dB. The 67NR tumors had a signal intensity of 50 ± 12.3 dB compared to the signal intensity of 12.0 ± 2.6 dB for the controls.

The degree of VEGFR2 expression on the two tumor types was also determined by immunoblotting and histochemistry (9). The 4T1 cell tumors exhibited a lower expression of VEGFR2 compared to the 67NR tumors. The vasculature of the two tumor types was also assessed by injecting fluoroscein isothiocynate-conjugated tomato lectin into the jugular vein of the mice 24 h after ultrasonography (9). The dye was allowed to circulate for 5 min, and then the mice were euthanized for resection of the tumors. This dye detects only functional blood vessels, and an increased number of blood vessels were observed in the 67NR tumors compared to those derived from the 4T1 cells. The investigators concluded that the ultrasound signal intensities observed with the tumors from the two cell lines correlated with the degree of VEGFR2 expression observed by immunoblotting and histochemistry.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2+sonography+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2+sonography+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VEGFR2+sonography+Human)]

No references are currently available.

## References

1 Shibuya M. (2006). Vascular endothelial growth factor (VEGF)-Receptor2: its biological functions, major signaling pathway, and specific ligand VEGF-E. Endothelium.
2 Plate K. (2001). From angiogenesis to lymphangiogenesis. Nat Med.
3 Carmeliet P., Moons L., Luttun A., Vincenti V., Compernolle V., De Mol M., Wu Y., Bono F., Devy L., Beck H., Scholz D., Acker T., DiPalma T., Dewerchin M., Noel A., Stalmans I., Barra A., Blacher S., Vandendriessche T., Ponten A., Eriksson U., Plate K.H., Foidart J.M., Schaper W., Charnock-Jones D.S., Hicklin D.J., Herbert J.M., Collen D., Persico M.G. (2001). Synergism between vascular endothelial growth factor and placental growth factor contributes to angiogenesis and plasma extravasation in pathological conditions. Nat Med.
4 Shibuya M., Claesson-Welsh L. (2006). Signal transduction by VEGF receptors in regulation of angiogenesis and lymphangiogenesis. Exp Cell Res.
5 Baillie R., Carlile J., Pendleton N., Schor A.M. (2001). Prognostic value of vascularity and vascular endothelial growth factor expression in non-small cell lung cancer. J Clin Pathol.
6 Schor A.M., Pendleton N., Pazouki S., Smither R.L., Morris J., Lessan K., Heerkens E., Chandrachud L.M., Carmichael G., Adi M., Chisholm D.M., Stevenson H. (1998). Assessment of vascularity in histological sections: effects of methodology and value as an index of angiogenesis in breast tumours. Histochem J.
7 Mazumdar M., Smith A., Schwartz L.H. (2004). A statistical simulation study finds discordance between WHO criteria and RECIST guideline. J Clin Epidemiol.
8 Schwartz L.H., Colville J.A., Ginsberg M.S., Wang L., Mazumdar M., Kalaigian J., Hricak H., Ilson D., Schwartz G.K. (2006). Measuring tumor response and shape change on CT: esophageal cancer as a paradigm. Ann Oncol.
9 Lyshchik A., Fleischer A.C., Huamani J., Hallahan D.E., Brissova M., Gore J.C. (2007). Molecular imaging of vascular endothelial growth factor receptor 2 expression using targeted contrast-enhanced high-frequency ultrasonography. J Ultrasound Med.
10 Ellegala D.B., Leong-Poi H., Carpenter J.E., Klibanov A.L., Kaul S., Shaffrey M.E., Sklenar J., Lindner J.R. (2003). Imaging tumor angiogenesis with contrast ultrasound and microbubbles targeted to alpha(v)beta3. Circulation.
11 Weller G.E., Wong M.K., Modzelewski R.A., Lu E., Klibanov A.L., Wagner W.R., Villanueva F.S. (2005). Ultrasonic imaging of tumor angiogenesis using contrast microbubbles targeted via the tumor-binding peptide arginine-arginine-leucine. Cancer Res.